# N-[2-(N-(2-mercaptoethyl)) amino ethyl]-N-(2-mercaptoethyl)-3,5-dimethylacetamide amantadine-technetium

Chemical name: | N-[2-(N-(2-mercaptoethyl)) amino ethyl]-N-(2-mercaptoethyl)-3,5-dimethylacetamide amantadine-technetium | [image]
Abbreviated name: | ^99m^Tc-NCAM | [image]
Synonym: | | [image]
Agent Category: | Compounds | [image]
Target: | N-methyl-D-aspartate receptor (NMDAR) | [image]
Target Category: | Receptors | [image]
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging | [image]
Source of signal / contrast: | ^99m^Tc | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structures of ^99m^Tc-NHAM (upper) and ^99m^Tc-NCAM (lower)

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=NMDA%20receptor%20and%20imaging)]

N-[2-(N-(2-mercaptoethyl)) amino ethyl]-N-(2-mercaptoethyl)-3,5-dimethylacetamide amantadine-technetium (^99m^Tc-NCAM) and 1-[N-[N-(2-mercaptoethyl)]-N-[2-[N-(2-mercaptoethyl) amino] ethyl] aminoethyl] amino-3,5-dimethyladmantane-technetium (^99m^Tc-NHAM) are two memantine derivatives synthesized by Zhou et al. for imaging of N-methyl-D-aspartate receptors (NMDARs) (1).

NMDARs are oligomeric ligand-gated, voltage-dependent ion channels formed by the assembly of a NR1 subunit and various NR2 subunits. NR1 has eight subtypes and encodes the ion channel, while NR2 has four subtypes (NR2A, NR2B, NR2C and NR2D) and mediates the fast excitatory neurotransmission in combination with NR1 (2). Recently the NR3 subunit (two subtypes, NR3A and NR3B) has been shown to combine with NR1 and NR2 to functional heterotrimers (3). In terms of agonist requirement and channel operation, the three subunit families exhibit distinct properties; NR1 and NR3 require glycine as the agonist and have no binding site for glutamate, whereas NR2 is activated by glutamate. Opening of the ion channel is dependent on the voltage state of the cell membrane as well as the binding of dual ligands; glutamate binds to a site on the NR2 subunit, and glycine or D-serine binds to a modulatory site on the NR1 subunit (2, 4). NMDARs present in both intra- and extra-synaptic areas, with a higher density within the synapse. The extra-synaptic NMDARs have been proposed to mediate excitotoxicity, while intra-synaptic NMDARs appear to be neuroprotective (5).

NMDARs have been a drug target for >25 years for neurological and psychiatric indications (2). A large number of mediators have been developed by targeting different modulatory sites on the NMDARs. With better understanding of the NMDAR pathophysiology, the therapeutic concept with channel mediators has changed over the years. As reviewed by Koller and Urwyler, the most important recent strategies aiming for inhibition of NMDAR-mediated neurotransmission is to avoid full receptor blockade while allowing a low degree of normal receptor function for safety reasons (2). To this aim, approaches include blocking the channel with compounds of low affinity, antagonizing receptor activity with highly potent NR2B ligands, partial agonism at the glutamate or glycine binding site, and improvement of pharmacokinetic properties of well established, safe antagonists by deuteration (2, 6).

Molecular imaging with radiotracers has been used to map the changes in the density of NMDARs in specific regions of brain and to establish receptor occupancy of a drug that may facilitate drug development and dose optimization. Because of the considerable number of binding sites (especially the channel pore, the glycine site, and the NR2B subunit), the NMDAR complex offers opportunities to develop imaging probes by targeting different sites (1, 7, 8). In general, most probes either have unfavorable pharmacokinetics or exhibit less specific binding, failing to reflect the distribution and density of NMDARs in different regions of brain. Memantine is a partial NMDAR antagonist approved in the United States and Europe for the treatment of moderate to severe Alzheimer’s disease. By acting at the channel pore, memantine preferentially blocks excessive NMDAR activity without disrupting its normal activity. Zhou et al. synthesized ^99m^Tc-NCAM and ^99m^Tc-NHAM with memantine as the lead compound (1). This chapter summarizes the data obtained with ^99m^Tc-NCAM and ^99m^Tc-NHAM.

### Related Resource Links:

NMDAR-related agents (http://www.ncbi.nlm.nih.gov/books/?term=N-methyl-D-aspartate+receptor+%28NMDAR%29+AND+micad%5bbook%5d&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books) in MICAD

Nucleotide (http://www.ncbi.nlm.nih.gov/nuccore?term=N-methyl-D-aspartate%20receptor%20%28NMDAR%29) and protein (http://www.ncbi.nlm.nih.gov/protein?term=N-methyl-D-aspartate%20receptor%20%28NMDAR%29) sequences of NMDAR

NMDAR-related articles (http://www.ncbi.nlm.nih.gov/omim?term=N-methyl-D-aspartate%20receptor%20%28NMDAR%29) in Online Mendelian Inheritance in Man

NMDAR-related clinical trials (http://clinicaltrials.gov/ct2/results?term=N-methyl-D-aspartate+receptor+%28NMDAR%29) in ClinicalTrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22516779)]

Zhou et al. described the synthesis of NCAM and NHAM in detail (1). ^99m^Tc-Labeling was performed in a 1.5-ml centrifuge tube containing sodium glucoheptonate, ethylenediamine tetraacetic acid (disodium salt), and NHAM or NCAM, followed by adding [^99m^Tc]NaTcO_4_ (37 MBq (1 mCi)) and fresh SnF_2_ solution. After the volume was adjusted to 1 ml with phosphate buffer, the mixture was heated for 45 min in boiling water and then cooled to room temperature. The radiochemical purity and entity of ^99m^Tc-NCAM and ^99m^Tc-NHAM were determined with high-performance liquid chromatography. The results showed that the radiochemical purity for both ^99m^Tc-NCAM and ^99m^Tc-NHAM was >95%, and >90% was retained after >6 h at room temperature. The retention times on chromatography were 11.27, 7.9, and 3.3 min for ^99m^Tc-NCAM, ^99m^Tc-NHAM, and [^99m^Tc][TcO_4_]^–^, respectively. The radiochemical yield and specific activity of the probes were not reported.

Partition coefficients with 1-octanol and phosphate-buffered saline were 1.79 ± 0.02 for ^99m^Tc-NCAM and 1.95 ± 0.05 for ^99m^Tc-NHAM, indicating that both probes were lipophilic.

Plasma protein binding was determined after incubation of each probe with 200 μl plasma for 3 h at 37°C, showing that ^99m^Tc-NCAM had slightly higher plasma protein binding than ^99m^Tc-NHAM (Table 1).

NMDAR binding kinetics was analyzed with NMDAR proteins prepared from Sprague-Dawley rat brain tissue (Table 1). The equilibrium dissociation constant (K_d_) was estimated with a saturation curve. The competitive binding of ^99m^Tc-NCAM and ^99m^Tc-NHAM with NMDAR was determined with two NMDAR-specific antagonists (ketamine and dizocilpine) and with a dopamine D_2_ and 5HT_1A_ receptor partial agonist (aripiprazole). The results showed that the specific binding of both ^99m^Tc-NCAM and ^99m^Tc-NHAM to NMDARs was blocked by ketamine and dizocilpine but not by aripiprazole. The 50% inhibitory concentration (IC_50_) was calculated according to the equation K_i_ = IC_50_/(1 + LT/K_d_), where K_i_ is the inhibition constant of ketamine or dizocilpine and LT is ligand concentration. The IC_50_ and K_i_ values indicated that both ^99m^Tc-NCAM and ^99m^Tc-NHAM had a high affinity for NMDARs (Table 2).

Table 1: Plasma protein binding and NMDAR binding kinetics of probes.

Plasma protein binding | Dose | ^99m^Tc-NHAM (%) | ^99m^Tc-NCAM (%)
| 3.7 MBq (0.1 mCi) | 62.5 | 79.6
| 0.74 MBq (0.02 mCi) | 58.1 | 81.3
| 0.148 MBq (0.004 mCi) | 63.2 | 83.5
K_d_ (mmol/l)* | N/A | 584.32 ± 87.27 | 701.21 ± 24.15
B_max_ (nmol/mg)* | N/A | 267.05 ± 22.06 | 62.47 ± 10.23

*Measured with NMDAR proteins prepared from Sprague-Dawley rat brain tissue

Table 2: Binding affinities of ^99m^Tc-NCAM and ^99m^Tc-NHAM.

| Ketamine (6 × 10^–1^ to 6 × 10^–11^ mol/L) | | Dizocilpine (6 × 10^–1^ to 6 × 10^–11^ mol/L)
| K_i_ | IC_50_ | K_i_ | IC_50_
^99m^Tc-NCAM* | 8.43 × 10^–6^ | 1.22 × 10^–5^ | 3.15 × 10^–8^ | 5.08 × 10^–8^
^99m^Tc-NHAM* | 9.28 × 10^–7^ | 9.46 × 10^–6^ | 2.43 × 10^–8^ | 3.69 × 10^–8^

*Measured with NMDAR proteins prepared from Sprague-Dawley rat brain tissue

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22516779)]

Cell uptake of ^99m^Tc-NHAM and ^99m^Tc-NCAM was measured after incubation of SH-SY5Y cell suspension (a human neuroblastoma cell line) (4.0 × 10^5^ cells/ml) with 0.185 MBq (0.05 mCi) ^99m^Tc-NHAM or ^99m^Tc-NCAM for different times. The protective effect of the precursors (NCAM and NHAM) on glutamate (5 mmol/L)-induced SH-HY5Y cell injury was also evaluated (1).

The data showed that the SH-HY5Y cell uptake of both ^99m^Tc-NHAM and ^99m^Tc-NCAM was significantly higher than that of [^99m^Tc]NaTcO_4_, peaking at 2.7% and 3.8% of added radioactivity, respectively, at 60 min. The cell uptake of both complexes then decreased slowly with prolonged incubation. Uptake of [^99m^Tc]NaTcO_4_ by SH-HY5Y cells was only 1%, and this value did not change as incubation time was extended. The precursors (NCAM, NHAM, and memantine) exhibited a protective effect on glutamate (at high concentrations)-induced cell death, showing that the survival of cells treated with NHAM, NCAM, and memantine was 159%, 143%, and 151%, respectively, compared to that of cells treated with glutamate alone.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22516779)]

Biodistribution of the ^99m^Tc-NCAM and ^99m^Tc-NHAM was studied in normal Kunming mice after tail vein injection of ~10 MBq (0.27 mCi) ^99m^Tc-NCAM or ^99m^Tc-NHAM (n = 5 mice/time point per agent) (1). Accumulation in organs and brain regions of interest was expressed as percentage of injected dose per gram tissue (% ID/g). The cortex (especially the parietal lobe) and the hippocampus were considered to be the target regions because of the highest density of NMDARs in these areas, and the cerebellum (CB) was considered to be the nontarget region because of the lowest density of NMDARs in CB.

Zhou et al. reported the detailed data of the probe uptake over time (see Figures 5 and 6 in reference (1)). Both ^99m^Tc-NCAM and ^99m^Tc-NHAM exhibited good penetration into the brain, reaching 1.23% and 1.47% ID/g, respectively, at 5 min after injection. For ^99m^Tc-NCAM, the highest regional uptake was observed in the cortex and hippocampus, followed by the striatum, and the lowest uptake was found in the CB. The frontal lobe/CB and hippocampus/CB ratios peaked at ~2.98 and 2.52, respectively, at 60 min after injection. In contrast, ^99m^Tc-NHAM showed random distribution throughout the brain without clear regional targeting. In the peripheral organs, high initial uptake was seen in the spleen and lungs for ^99m^Tc-NCAM and in the liver and kidneys for ^99m^Tc-NHAM, both of which then decreased quickly over time. No blocking studies were reported.

The blood kinetics of ^99m^Tc-NCAM was analyzed after injection into six mice via tail vein (1). The pharmacokinetic equation was C = 5.492e−^0.3141t^ + 0.275e−^0.0042t^. The absorption half-life of ^99m^Tc-NCAM was 2.2 min.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22516779)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=22516779)]

No references are currently available.

## References

1 Zhou, X., Zhang, J., Yan, C., Cao, G., Zhang, R., Cai, G., Jiang, M., and Wang, S. Preliminary studies of (99m)Tc-memantine derivatives for NMDA receptor imaging. Nucl Med Biol. 2012
2 Koller, M. and Urwyler, S. Novel N-methyl-D-aspartate receptor antagonists: a review of compounds patented since 2006. Expert Opin Ther Pat. 2010: 20(12): 1683-702.
3 Bergeron R., Coyle J.T. (2012). NAAG, NMDA receptor and psychosis. Curr Med Chem.
4 Laruelle M., Kegeles L.S., Abi-Dargham A. (2003). Glutamate, dopamine, and schizophrenia: from pathophysiology to treatment. Ann N Y Acad Sci.
5 Fitzgerald P.J. (2012). The NMDA receptor may participate in widespread suppression of circuit level neural activity, in addition to a similarly prominent role in circuit level activation. Behav Brain Res.
6 Laruelle, M., Frankle, W.G., Narendran, R., Kegeles, L.S., and Abi-Dargham, A. Mechanism of action of antipsychotic drugs: from dopamine D(2) receptor antagonism to glutamate NMDA facilitation. Clin Ther. 2005: 27 Suppl A: S16-24.
7 Stone J.M. (2009). Imaging the glutamate system in humans: relevance to drug discovery for schizophrenia. Curr Pharm Des.
8 Sobrio F., Gilbert G., Perrio C., Barre L., Debruyne D. (2010). PET and SPECT imaging of the NMDA receptor system: an overview of radiotracer development. Mini Rev Med Chem.